# ^68^Ga-Glutamate peptide-3 aminoethyl estradiol

Chemical name: | ^68^Ga-Glutamate peptide-3 aminoethyl estradiol | [image]
Abbreviated name: | ^68^Ga-GAP-EDL | [image]
Synonym: | | [image]
Backbone: | Estradiol | [image]
Target: | Estrogen receptor | [image]
Mechanism: | Receptor-ligand binding | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal: | ^68^Ga | [image]
Activation: | Not required | [image]
Studies: | - In vitro; - Rodents | Structure of GAP-EDL. The exact location of ^68^Ga in the structure is unknown.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GAP-EDL)]

Approximately 10% of women of reproductive age are affected by endometriosis, a gynecological disorder (1). Painful periods, pelvic pain, and infertility are often associated with endometriosis. Although a variety of mechanisms, including the roles of different cytokines, growth factors, and hormones, have been proposed in the development of endometriosis, the exact etiology and epidemiology of this condition is unclear (1-3). Menstruation in the opposite direction with spillage of viable endometrial cells into the peritoneum is often observed in cycling women (4). Adhesion, proliferation, and spread of the shed endometrial cells to the peritoneum are believed to support the development of endometriosis (5-7). Endometriosis is usually detected by a surgical technique such as a laparoscopy. Performing such a procedure on patients with infertility is often complex, and it provides information only about the morphological and anatomical changes in the tissue (8). Moreover, endometriosis usually progresses or recurs after surgery, and any relief to the patient is temporary (9).

Because the prevalence and progression of endometriosis cannot be studied in humans without a laparoscopy, non-primate and primate animal models, including rabbits, have been used to investigate this disease (10-12). It has also been shown that estrogen receptors (ER) are overexpressed in the uterine endometrium and endometriotic lesions in endometriosis (4). In an effort to develop a non-invasive method to detect endometriosis, Takahashi et al. explored the use of estrogen, an ER ligand, to image endometriosis induced in rabbits (8). For this, estradiol (EDL) was conjugated to a glutamate peptide (GAP), which contained 5–10 glutamic acid residues, to facilitate the chelation of radioactive gallium (^68^Ga) to obtain ^68^Ga-GAP-EDL to image endometriosis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Ga+GAP+EDL)]

The synthesis of ^68^Ga-GAP-EDL was performed as described by Takahashi et al. (8, 13). To start, estrone was dissolved in anhydrous ethanol. Sodium ethoxide and bromoacetonitrile were added to the solution and the mixture was heated under reflux for 3 h. The ethanol was allowed to evaporate completely and the residue was dissolved in ethyl acetate. The solution was washed with water and the organic layer was filtered after drying over magnesium sulphate. The ethyl actetate was evaporated under reduced pressure and the remaining solid product, 3-acetonitrile estradiol, was washed with ether. The yield of this reaction was 75%. The solid product was dissolved in tetrahydrofuran, and lithium aluminum hydride was added to the mixture and stirred for 4 h. The solvent was evaporated to yield a solid that was dissolved in ethyl acetate. This solution was washed with water, dried over magnesium sulphate, and filtered. The solvent was evaporated to obtain 3-cyanomethyl estrone (EDL) with a yield of 92%. The structure of EDL was confirmed by nuclear magnetic resonance.

For the synthesis of GAP-EDL, the sodium salt of GAP was converted to the acid form by the addition of 2 N hydrochloric acid (HCl). This solution was dialyzed to remove all the acid and freeze-dried to obtain the acidic form of GAP. The GAP acid was dissolved in dimethylformamide (DMF), and dicyclohexyl carbodiimide and 4-N,N-dimethyl aminopyridine were added to it. This mixture was stirred at room temperature for 2 days. The DMF was evaporated under reduced pressure; 1 N sodium bicarbonate was added to it and extracted with chloroform. The aqueous solution was dialyzed, filtered, and freeze-dried to obtain GAP-EDL. The percent yield of this reaction was not provided in the publication. The GAP-EDL complex contained 7% (weight/weight) EDL as determined by ultraviolet spectroscopy.

For the synthesis of ^68^Ga-GAP-EDL, ^68^Ga was eluted from a ^68^Ge/^68^Ga generator with 0.1 N HCl, and the acidic solution was passed through an anion resin cartridge to trap the ^68^Ga. The cartridge was washed with 4 N HCl and air-dried. The ^68^Ga was eluted as ^68^Ga-chloride (^68^GaCl_3_) from the cartridge with water, and the pH was adjusted to 4–5 with sodium hydroxide and sodium acetate. GAP-EDL in acetate buffer was added to the ^68^GaCl_3_ solution, and the reaction was completed by warming at 37°C for 20 min. Radiochemical purity of the product was determined by instant thin-layer chromatography. The Rf values for GAP-EDL and ^68^GaCl_3_ were reported to be 0.1 and 0.9, respectively. The radiochemical purity of the radiotracer was >95%. Specific activity of the radiotracer was not provided in the publication (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeled-GAP-EDL+in+vitro)]

The uptake of ^68^Ga-GAP-EDL was studied in the 13762 rat adenocarcinoma cell line (8), and accumulation of the radiopharmaceutical in these cells was shown to increase with time. Addition of cold estrone (estradiol) inhibited the uptake in a dose-dependent manner. This indicated that the uptake of ^68^Ga-GAP-EDL in the cells was an ER-mediated process.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gap-edl+rodentia)]

No publications are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gap-edl+non+primate+mammals)]

The uptake of ^68^Ga-GAP-EDL was investigated in rabbits with induced endometriosis (8). Endometrial tissues were implanted in the rabbits, and the implanted endometrial tissue was microscopically visible in the animals after 8 weeks. The uptake of ^68^Ga-GAP-EDL by the rabbits was investigated with and without the treatment of tamoxifen, a competitive inhibitor of estrogen for binding to the ER. A cross-sectional review of the coronal and sagittal images taken by positron emission tomography showed that the endometrial implant tissue could be differentiated from the skeletal, hepatobiliary, and urinary uptake of the label. Prior treatment of the animals with tamoxifen resulted in the inhibition of label uptake by the endometrial tissue. This demonstrated that the uptake of ^68^Ga-GAP-EDL in the endometrial implants was ER-mediated. From this observation, the investigators suggested that ^68^Ga-GAP-EDL can be used as a non-invasive imaging agent for the detection and monitoring of endometriosis and other diseases associated with the overexpression of ER, such as breast cancer .

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+gap-edl+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeled+GAP+EDL+humans)]

No publications are currently available.

## References

1 Lebovic D.I., Mueller M.D., Taylor R.N. (2001). Immunobiology of endometriosis. Fertil Steril.
2 Cramer, D.W. and S.A. MissmerThe epidemiology of endometriosis. Ann N Y Acad Sci, 2002955: p. 11-22; discussion 34-6, 396-406.
3 Hever A., Roth R.B., Hevezi P., Marin M.E., Acosta J.A., Acosta H., Rojas J., Herrera R., Grigoriadis D., White E., Conlon P.J., Maki R.A., Zlotnik A. (2007). Human endometriosis is associated with plasma cells and overexpression of B lymphocyte stimulator. Proc Natl Acad Sci U S A.
4 Leyendecker G., Herbertz M., Kunz G., Mall G. (2002). Endometriosis results from the dislocation of basal endometrium. Hum Reprod.
5 Halme J., Hammond M.G., Hulka J.F., Raj S.G., Talbert L.M. (1984). Retrograde menstruation in healthy women and in patients with endometriosis. Obstet Gynecol.
6 Kruitwagen R.F., Poels L.G., Willemsen W.N., de Ronde I.J., Jap P.H., Rolland R. (1991). Endometrial epithelial cells in peritoneal fluid during the early follicular phase. Fertil Steril.
7 Evers J.L. (1996). The defense against endometriosis. Fertil Steril.
8 Takahashi N., Yang D.J., Kurihara H., Borne A., Kohanim S., Oh C.S., Mawlawi O., Kim E.E. (2007). Functional Imaging of Estrogen Receptors with Radiolabeled-GAP-EDL in Rabbit Endometriosis Model. Acad Radiol.
9 DeCherney A.H. (1992). Endometriosis: recurrence and retreatment. Clin Ther.
10 D'Hooghe T.M., Bambra C.S., Raeymaekers B.M., De Jonge I., Lauweryns J.M., Koninckx P.R. (1995). Intrapelvic injection of menstrual endometrium causes endometriosis in baboons (Papio cynocephalus and Papio anubis). Am J Obstet Gynecol.
11 Schenken R.S., Asch R.H. (1980). Surgical induction of endometriosis in the rabbit: effects on fertility and concentrations of peritoneal fluid prostaglandins. Fertil Steril.
12 Steinleitner A., Lambert H., Suarez M., Serpa N., Roy S. (1991). Immunomodulation in the treatment of endometriosis-associated subfertility: use of pentoxifylline to reverse the inhibition of fertilization by surgically induced endometriosis in a rodent model. Fertil Steril.
13 Takahashi N., Yang D.J., Kohanim S., Oh C.S., Yu D.F., Azhdarinia A., Kurihara H., Zhang X., Chang J.Y., Kim E.E. (2007). Targeted functional imaging of estrogen receptors with 99mTc-GAP-EDL. Eur J Nucl Med Mol Imaging.